# N'-Fluorescein-N''-[4-O-(β-D-glucopyranuronic acid)-3-difluoromethylphenyl]-S-methylthiourea (FITC-TrapG) and N'-(p-aminophenyl)thioether of IR-820-N''-[4-O-(β-D-glucopyranuronic acid)-3-difluoromethylphenyl]-S-methylthiourea (NIR-TrapG)

Chemical name: | N'-Fluorescein-N''-[4-O-(β-D-glucopyranuronic acid)-3-difluoromethylphenyl]-S-methylthiourea (FITC-TrapG) and N'-(p-aminophenyl)thioether of IR-820-N''-[4-O-(β-D-glucopyranuronic acid)-3-difluoromethylphenyl]-S-methylthiourea (NIR-TrapG)
Abbreviated name: | FITC-TrapG and NIR-TrapG
Synonym:
Agent Category: | Compounds
Target: | β-Glucuronidase (βG; β-GUS)
Target Category: | Enzyme
Method of detection: | Optical imaging (near-infrared imaging for NIR-TrapG and fluorescence imaging for FITC-TrapG)
Source of signal / contrast: | IR-820 (NIR) and fluorescein isothiocynate (FITC)
Activation: | Yes
Studies: | - In vitro; - Rodents | Structures not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Glucuronidase&cmd=DetailsSearch)]

The β-glucuronidase (βG; EC 3.2.1.31) is a lysosomal enzyme that catalyzes the hydrolysis of β-glucuronic acid residues from the cell-surface glycosaminoglycans for normal reconstruction of the extracellular matrix (ECM) (1), and the enzyme is believed to participate in the processes of angiogenesis, cancer metastasis, and inflammation (2). The βG is known to activate prodrugs (PDs) for the treatment of cancer. βG also has been used to track the path of gene delivery vehicles, and there is evidence that it can be used as a biomarker to detect cancerous tumors (3). Normal tissues have low levels of βG in the ECM, but tissues under pathological stress, such as bacterial infection, fibrosis, or malignancy, show elevated levels of the enzyme (4). As a result of cell lysis, intracellular βG is released from the necrotic parts of neoplastic tumors, and its activity in these lesions has been utilized for the in situ activation of anti-cancer PDs to treat cancers (1). Because chemotherapeutic anti-cancer drugs are nonselectively toxic to healthy cells, they are generally of limited efficacy to the patient due to their undesirable side effects on the normal biological systems. The conversion of a toxic drug into a non-toxic PD that can be activated only under specific conditions (e.g., by enzyme catalysis or chemical hydrolysis) would facilitate drug activation only in tissues that provide the specialized microenvironment and improve its concentration and efficacy at the desired location in the body (5, 6). For example, glucuronide PDs (drugs that are linked to a glucuronic acid moiety with or without a linker) have been shown to have superior anti-tumor activity compared with the parent drugs because the activated drugs are released from the PDs by the βG activity in a site-specific manner (7, 8).

βG activity varies among individuals, and its expression or accumulation in tumor tissues may change depending on the type of neoplasm or location in the body (1, 9). Two [^18^F]fluoride-labeled probes, 1-O-(4-(2-[^18^F]fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate ([^18^F]-FEAnGA) (1, 4, 10) and its methyl ester (([^18^F]-FEAnGA-Me) (11), were synthesized as PDs and used with positron emission tomography (PET) to detect and visualize βG activity in tumors and inflamed tissues in rodents. Although [^18^F]-FEAnGA or [^18^F]-FEAnGA-Me could detect the βG activity and distinguish cancerous tumors or inflamed tissues from the surrounding normal tissues, only modestly higher levels of radioactivity were observed to accumulate with either tracer in the tumorous or inflamed areas compared with the surrounding tissues. The investigators concluded that low accumulation of label in the lesions was probably due to rapid clearance of the radiochemicals from the body through the kidneys (1, 11). A nonfluorescent substrate, fluorescein di-β-D-glucuronide (FDGlcU), was developed to determine the expression of βG with optical imaging in the various tissues of mice (12). However, the signals generated with FDGlcU could be detected only in the superficial tissues of small animals (such as rodents), suggesting that the low depth of light penetration in tissues would limit its application for the visualization of deep-seated tumors in animals or humans (3). Therefore, two βG activity-based optical probes were developed and evaluated to detect the enzyme in deep tissues (e. g. liver) of mice (3). To generate the probes, difluoromethylphenol-glucuronide (TrapG) was linked to either a near-infrared (NIR) dye (IR-820, λ_ex_/λ_em_ = 490 nm/525 nm; NIR-TrapG) or a fluorescein isothiocyanate (FITC, λ_ex_/λ_em_ = 710 nm/835 nm; FITC-TrapG) moiety to visualize the enzyme activity in the NIR or the visible ranges of light, respectively. The mechanism of action of these probes has been explained and illustrated by Cheng et al. (3). Briefly, with NIR-Trap as the example, the βG hydrolyzes the glucuronyl bond in the NIR-TrapG molecule and produces a quinine methide intermediate that contains the NIR dye moiety. The intermediate complex is highly reactive toward nucleophilic side chains of amino acids (such as in lysine) in proteins that are close to the βG-expressing sites and results in crosslinking of the fluorochrome to these molecules. The signal generated from the fluorochrome can then be detected with an appropriate optical imaging system. The biodistribution of NIR-TrapG and FITC-TrapG was investigated in mice bearing CT26 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2638&Template=cellBiology) tumors (control) or CT26/mβG cell tumors (these are derivatives of the CT26 cells and express βG on the cell membrane surface) (3). The probes were also evaluated for the detection of subcutaneous and deep tissue (hepatic) tumors in these animals.

### Related Resource Links

Other prodrug chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Prodrug+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Homo sapiens β-GUS protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_000181.3)

Prodrug-related clinical trials (http://clinicaltrials.gov/ct2/results?term=prodrugs)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20synthesis%22&cmd=DetailsSearch)]

The synthesis of NIR-TrapG and FITC-TrapG has been described by Cheng et al. (3). Briefly, FITC and the IR-820 dye were obtained from commercial sources and linked to a glucuronide residue through difluoromethylphenol (the trapping moiety) to obtain the NIR-TrapG and FITC-TrapG probes, respectively. The mass and structure of the final products were confirmed with liquid chromatography-mass spectrometry and nuclear magnetic resonance, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20In%20Vitro%20Studies%22&cmd=DetailsSearch)]

Using an ELISA assay, increasing concentrations of FITC-TrapG were shown to be activated by purified βG enzyme or by intact CT26/mβG cells (3). The absorbance (at 405 nm) of the ELISA assay increased from ~0.1 unit in absence of FITC-TrapG to 2.0 units in presence of 40 μg/mL of the FITC conjugate. A similar trend was observed with the intact CT26/mβG cells (absorbance at 405 nm was ~0.15 units without FITC-TrapG and increased to ~1.25 units in presence of 40 μg/mL of the FITC conjugate). Western blot analysis showed that activated FITC-TrapG could cross-link the nucleophile groups of both bovine serum albumin (BSA) and purified Escherichia coli βG (eβG) with FITC (3). It has been shown that FITC-TrapG did not label the BSA in absence of the eβG. These studies demonstrated that the probe is a suitable substrate for the eβG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20rodentia%22&cmd=DetailsSearch)]

FITC-TrapG and NIR-TrapG were evaluated for the detection of βG activity in subcutaneous CT26 cell and CT26/mβG tumors in the left and right flanks, respectively, of BALB/c nude mice (n = 3 animals) (3). The animals were injected intravenously with either ~0.833 μmol FITC-TrapG or ~0.12 μmol NIR-TrapG, and the fluorescence intensity (FI) values from the tumors and other organs were recorded at 24, 48, and 72 h postinjection (p.i.) with an acquisition time of 10 s at each time point. FI values of the tumors were calculated and reported as photons per s^1^·cm^2^·sr^1^ as described by Cheng et al. (3). With FITC-TrapG, the FI values of the CT26/mβG cell tumors were 4.59-, 3.86-, and 2.86-fold higher than that of the control CT26 cell tumors at 24, 48, and 72 h p.i., respectively. Presence or absence of βG activity in the tumors was confirmed histologically as described by Cheng et al. (3). The FI values of the CT26/mβG cell tumors with NIR-TrapG at 24, 48, and 72 h p.i. were 4.25-, 4.92-, and 5.21-fold higher, respectively, than the control CT26 cell tumors. These results indicated that the NIR-TrapG probe was superior to the FITC-TrapG probe for detection of the βG activity because it generated higher a FI with the CT26/mβG tumors. Similar results were obtained from the biodistribution study (n = 3 mice) with both probes (3). Apart from accumulation in the CT26/mβG tumors, optical signals from the FITC-TrapG and the NIR-TrapG probes were detected in the liver, kidneys, intestines, and bladder of the animals. This indicated that the TrapG probe derivatives were eliminated from the body through the urinary and the hepatobiliary routes in these animals.

The FITC-TrapG and NIR-TrapG probes were also evaluated for the visualization of βG activity in CT26 cell (control) or CT26/mβG cell tumors transplanted under the capsule of the liver in mice (n = 3 animals/probe) (3). The animals were injected with FITC-TrapG or NIR-TrapG as before, and whole-body fluorescence signals were recorded from the animals under anesthesia at 24 p.i. After acquiring the images, the livers were extracted from the animals for ex vivo imaging to confirm the presence of the dyes in the organs. Whole-body images showed that NIR signals were detected in the livers of mice injected with the NIR-TrapG probe, whereas no FITC signals were observed in the livers of mice injected with the FITC-TrapG probe. However, FITC signals were visible in the livers only when ex vivo images of the organs were acquired.

From these studies, the investigators concluded that the NIR-TrapG probe was suitable for the noninvasive imaging of βG activity in deep tissues of rodents (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20Other%20Non-Primate%20Mammals%22&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20Non-Human%20Primates%22&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22NIR-TrapG%20Human%20Studies%22&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Antunes I.F., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). In Vivo Evaluation Of 1-o-(4-(2-fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-o-beta-d-glucopyronurona te: A Positron Emission Tomographic Tracer For Imaging beta-glucuronidase Activity In A Tumor/inflammation Rodent Model. Mol Imaging.
2 Gandhi N.S., Freeman C., Parish C.R., Mancera R.L. (2012). Computational analyses of the catalytic and heparin-binding sites and their interactions with glycosaminoglycans in glycoside hydrolase family 79 endo-beta-D-glucuronidase (heparanase). Glycobiology.
3 Cheng T.C., Roffler S.R., Tzou S.C., Chuang K.H., Su Y.C., Chuang C.H., Kao C.H., Chen C.S., Harn I.H., Liu K.Y., Cheng T.L., Leu Y.L. (2012). An activity-based near-infrared glucuronide trapping probe for imaging beta-glucuronidase expression in deep tissues. J Am Chem Soc.
4 Antunes I.F., Haisma H.J., Elsinga P.H., Dierckx R.A., de Vries E.F. (2010). Synthesis and evaluation of [18F]-FEAnGA as a PET Tracer for beta-glucuronidase activity. Bioconjug Chem.
5 Antunes I.F., Haisma H.J., de Vries E.F. (2008). Tumor-specific activation of prodrugs: is there a role for nuclear medicine?. Nucl Med Commun.
6 Huttunen K.M., Raunio H., Rautio J. (2011). Prodrugs--from serendipity to rational design. Pharmacol Rev.
7 Thomas M., Clarhaut J., Tranoy-Opalinski I., Gesson J.P., Roche J., Papot S. (2008). Synthesis and biological evaluation of glucuronide prodrugs of the histone deacetylase inhibitor CI-994 for application in selective cancer chemotherapy. Bioorg Med Chem.
8 Renoux B., Legigan T., Bensalma S., Chadeneau C., Muller J.M., Papot S. (2011). A new cyclopamine glucuronide prodrug with improved kinetics of drug release. Org Biomol Chem.
9 Tzou S.C., Roffler S., Chuang K.H., Yeh H.P., Kao C.H., Su Y.C., Cheng C.M., Tseng W.L., Shiea J., Harm I.H., Cheng K.W., Chen B.M., Hwang J.J., Cheng T.L., Wang H.E. (2009). Micro-PET imaging of beta-glucuronidase activity by the hydrophobic conversion of a glucuronide probe. Radiology.
10 Antunes I.F., Doorduin J., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). 18F-FEAnGA for PET of beta-Glucuronidase Activity in Neuroinflammation. J Nucl Med.
11 Antunes, I.F., H.J. Haisma, P.H. Elsinga, J.W. Sijbesma, A.V. Waarde, A.T. Willemsen, R.A. Dierckx, and E.F. de Vries, In vivo evaluation of [(18)F]FEAnGA-Me: a PET tracer for imaging beta-glucuronidase (beta-GUS) activity in a tumor/inflammation rodent model. Nucl Med Biol, 2012
12 Su Y.C., Chuang K.H., Wang Y.M., Cheng C.M., Lin S.R., Wang J.Y., Hwang J.J., Chen B.M., Chen K.C., Roffler S., Cheng T.L. (2007). Gene expression imaging by enzymatic catalysis of a fluorescent probe via membrane-anchored beta-glucuronidase. Gene Ther.